# anti-1-Amino-3-[^18^F]fluorocyclobutane-1-carboxylic acid

Chemical name: | anti-1-Amino-3-[^18^F]fluorocyclobutane-1-carboxylic acid
Abbreviated name: | anti-[^18^F]FACBC, anti-3-[^18^F]FACBC
Synonym:
Agent category: | Compound
Target: | L-type amino acid transporter
Target category: | Transporter
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=facbc%5BAll%20Fields%5D)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain (3). These amino acids are composed of naturally occurring amino acids, such as, L-[^11^C]leucine, L-[^11^C]methionine, and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. There are also ^123^I-labeled amino acids used in imaging in oncology (4-6).The natural amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and retained in tumor cells because of their higher metabolic pathways, including incorporation into proteins than most normal cells (4). L-[^11^C]Methionine (http://www.ncbi.nlm.nih.gov/books/bv.fcgi?rid=micad.chapter.MET11C) and [^18^F]fluorotyrosine (http://www.ncbi.nlm.nih.gov/books/bv.fcgi?rid=micad.chapter.FMT18F) have been widely used in the detection of tumors. On the other hand, the non-natural amino acids are not metabolized. Their uptakes are through both the L-type transporter and the energy-dependent A-type transporter (7). Therefore, they can be accumulated intracellularly in high concentrations. anti-1-Amino-3-[^18^F]fluorocyclobutane-1-carboxylic acid (anti-[^18^F]FACBC) was shown to have a high tumor/brain ratio (8). Therefore, anti-[^18^F]FACBC could be a useful tracer in PET tumor imaging.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D)
- Gene information in NCBI (L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in OMIM (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+synthesis)]

Nucleophilic fluorination of syn-1-t-butyl-carbamate-3-trifluromethanesulfonoxy-1-cyclobutane-1-carboxylic acid methyl ester with K[^18^F]F/Kryptofix2.2.2 and subsequent hydrolysis and purification provided a radiosynthesis yield of 12% of anti-[^18^F]FACBC at the end of bombardment (8). A radiochemical purity of 99% was obtained. The total synthesis time was 60 min. An automated radiosynthesis of anti-[^18^F]FACBC was reported with a radiosynthesis yield of 24% and a radiochemical purity of 99% (9). The specific activity was 137-192 GBq/mmol (3.7-5.2 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+in+vitro)]

anti-[^18^F]FACBC showed a fast-increasing uptake into human DU-145 prostate tumor cells in the first 5 min in culture with ~6% injected dose (10)/10^5^ cells, followed by a peak (~8% ID/10^5^ cells) at 15 min and a gradual decrease to 3% ID/10^5^ cells at 60 min (10). The uptake was blocked by the presence of excess natural amino acids to <0.2% ID/10^5^ cells. On the other hand, uptake of 2-[^18^F]fluoro-2-deoxy-D-glucose ([^18^F]FDG (http://www.ncbi.nlm.nih.gov/books/bv.fcgi?rid=micad.chapter.FDG)) increased with time from ~1% ID/10^5^ cells at 5 min to 9% ID/10^5^ cells at 60 min. The uptake was blocked by the presence of excess glucose to <0.5% ID/10^5^ cells.

Yu et al. (11) showed that anti-[^18^F]FACBC uptake into rat 9L gliosarcoma tumor cells in culture was reduced by 76%, 6%, and 98% by the presence of 10 mM of BCH, MeAIB, and ACS, respectively. The data suggest that anti-[^18^F]FACBC is predominantly a L-type transporter substrate .

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+rodentia)]

Uptake of anti-[^18^F]FACBC and [^18^F]FDG were compared in rats implanted intracerebrally with 9L gliosarcoma (8). Accumulation of anti-[^18^F]FACBC in the spleen, lungs, liver, and kidneys was greater than in the heart, tumor, blood, and brain at 5 min after injection. The uptake in the brain (0.11% ID/g) was low and increased slightly to 0.26% ID/g at 60 min. The uptake in the tumor increased from 0.62% ID/g to 1.72% ID/g. Most of the other tissues showed a decrease in radioactivity at 60 min, except for the liver, which showed an increase. Accumulation of [^18^F]FDG in the kidneys, liver, heart, brain tumor and blood was from 0.91%ID/g to 1.3% ID/g at 5 min. However, there was little difference in the uptake between the brain and tumor at 5 min and 60 min. The tumor-to-brain ratio at 60 min was 6.6 and 0.84 for anti-[^18^F]FACBC and [^18^F]FDG, respectively.

Oka et al. (10) compared the biodistribution of anti-[^18^F]FACBC and [^18^F]FDG in rats transplanted with DU-145 tumor cells orthotopically in the prostate (OPCT). In the brain, heart, small intestine, testis, mesenteric lymph nodes, and urinary bladder, the accumulation of [^18^F]FDG was higher than that of anti-[^18^F]FACBC at 15 and 60 min after injection. On the other hand, anti-[^18^F]FACBC uptake into the liver, muscle, and pancreas was higher than [^18^F]FDG uptake into these organs at 15 and 60 min. The uptake of anti-[^18^F]FACBC (1.58 ± 0.40% ID/cm^3^) and [^18^F]FDG (1.48 ± 0.90% ID/cm^3^) into the prostate cancer tissue was similar at 60 min. In contrast, [^18^F]FDG (0.55 ± 0.18% ID/cm^3^) uptake into the normal prostate regions was significantly higher than anti-[^18^F]FACBC (0.37 ± 0.06% ID/cm^3^) (P < 0.05). The accumulation of anti-[^18^F]FACBC (3.09 ± 1.43% ID/cm^3^) was significantly lower than [^18^F]FDG (69.31 ± 16.55% ID/cm^3^) in the urinary bladder at 60 min (P < 0.05).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACBC+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=facbc%5BAll%20Fields%5D%20AND%20human)]

PET imaging using anti-[^18^F]FACBC was taken one week after a patient had undergone surgery to remove a tumor in the brain (8). The uptake of anti-[^18^F]FACBC in normal brain tissue was 21 nCi/ml and 29 nCi/ml at 5 min and 60 min, respectively. The uptake in tumor was 110 nCi/ml at 5 min and 130 nCi/ml at 60 min. Human dosimetry was estimated by Nye et al. (12) using the biodistribution data from 6 healthy volunteers. The liver received the highest dose of radioactivity, followed by the pancreas, heart wall, kidneys, and spleen. The effective dose equivalent is 0.0164 mSv/MBq (60.6 mrem/mCi).

Schuster et al. (13) studied 15 patients with a recent diagnosis of prostate carcinoma (n = 9) or suspected recurrence (n = 6) underwent 65-min dynamic PET/CT of the pelvis after injection of 300-410 MBq (8.1-11.1 mCi) anti-[^18^F]FACBC followed by static body images. In the 8 patients with newly diagnosed prostate carcinoma who underwent dynamic scanning, visual analysis correctly identified the presence or absence of focal cancer lesions in 40 of 48 prostate sextants. Pelvic nodal status correlated with anti-[^18^F]FACBC findings in 7 of 9 patients and was indeterminate in 2 of 9. Visual analysis was successful in identifying disease in all 4 patients with proven recurrence.

Savir-Baruch et al. (14) studied five patients with elevated prostate-specific antigen level after curative therapy for prostate carcinoma underwent 60-min dynamic PET/CT of the pelvis after injection of 193-340 MBq (5.2-9.3 mCi) anti-[^18^F]FACBC. Average standard uptake value (SUV) of malignant lesions was 4.3 ± 1.1 and 3.4 ± 0.8 at 5 and 20 min, respectively. The lesion/blood ratios were 3.0 ± 0.9 at 5 min, whereas lesions/urinary bladder ratio was 2.3 ± 1.4 at 20 min.

## References

1 Coleman R.E., Hoffman J.M., Hanson M.W., Sostman H.D., Schold S.C. (1991). Clinical application of PET for the evaluation of brain tumors. J Nucl Med.
2 Kaschten B., Stevenaert A., Sadzot B., Deprez M., Degueldre C., Del Fiore G., Luxen A., Reznik M. (1998). Preoperative evaluation of 54 gliomas by PET with fluorine-18-fluorodeoxyglucose and/or carbon-11-methionine. J Nucl Med.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
5 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
6 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
7 Palacin M., Estevez R., Bertran J., Zorzano A. (1998). Molecular biology of mammalian plasma membrane amino acid transporters. Physiol Rev.
8 Shoup T.M., Olson J., Hoffman J.M., Votaw J., Eshima D., Eshima L., Camp V.M., Stabin M., Votaw D., Goodman M.M. (1999). Synthesis and evaluation of [18F]1-amino-3-fluorocyclobutane-1-carboxylic acid to image brain tumors. J Nucl Med.
9 McConathy J., Voll R.J., Yu W., Crowe R.J., Goodman M.M. (2003). Improved synthesis of anti-[18F]FACBC: improved preparation of labeling precursor and automated radiosynthesis. Appl Radiat Isot.
10 Oka S., Hattori R., Kurosaki F., Toyama M., Williams L.A., Yu W., Votaw J.R., Yoshida Y., Goodman M.M., Ito O. (2007). A preliminary study of anti-1-amino-3-18F-fluorocyclobutyl-1-carboxylic acid for the detection of prostate cancer. J Nucl Med.
11 Yu W., Williams L., Camp V.M., Malveaux E., Olson J.J., Goodman M.M. (2009). Stereoselective synthesis and biological evaluation of syn-1-amino-3-[18F]fluorocyclobutyl-1-carboxylic acid as a potential positron emission tomography brain tumor imaging agent. Bioorg Med Chem.
12 Nye J.A., Schuster D.M., Yu W., Camp V.M., Goodman M.M., Votaw J.R. (2007). Biodistribution and radiation dosimetry of the synthetic nonmetabolized amino acid analogue anti-18F-FACBC in humans. J Nucl Med.
13 Schuster D.M., Votaw J.R., Nieh P.T., Yu W., Nye J.A., Master V., Bowman F.D., Issa M.M., Goodman M.M. (2007). Initial experience with the radiotracer anti-1-amino-3-18F-fluorocyclobutane-1-carboxylic acid with PET/CT in prostate carcinoma. J Nucl Med.
14 Savir-Baruch, B., D.M. Schuster, N. Jarkas, V.A. Master, P.T. Nieh, R.K. Halkar, J.A. Nye, M.M. Lewis, R.J. Crowe, R.J. Voll, V.M. Camp, L.M. Bellamy, D.L. Roberts, and M.M. Goodman, Pilot Evaluation of Anti-1-amino-2-[(18)F] fluorocyclopentane-1-carboxylic acid (anti-2-[(18)F] FACPC) PET-CT in Recurrent Prostate Carcinoma. Mol Imaging Biol, 2010